# [6-O-methyl-^11^C]Diprenorphine

Chemical name: | [6-O-methyl-^11^C]Diprenorphine
Abbreviated name: | [^11^C]DPN
Synonym: | [^11^C]Diprenorphine
Agent category: | Compound
Target: | Opioid receptors
Target category: | Receptor
Method of detection: | PET
Source of signal\contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20diprenorphine)]

Opioids such as morphine are commonly used analgesics in clinical practice. Three opioid receptors (mu, µ; delta, δ; and kappa, κ) that mediate opioid effects have been identified by molecular cloning: δ (enkephalin-preferring), κ (dynorphin-preferring), and µ (morphine and ß-endorphin-preferring) (1). Each type of opioid receptors consists of subtypes of receptors as suggested by pharmacological studies (2, 3). Their specificity and ubiquitous location are present in both the central and peripheral nervous system. The opioid receptors (G-protein coupled, resulting in decrease in adenylyl cyclase activity) play an important role in the regulation of analgesia, shock, appetite, thermoregulation, cardiovascular, mental and endocrine function (2-5). Although µ opioid receptors are the major receptor to mediate the analgesic effects of opioids, δ and κ receptors are also important in antinociception. Opioids have been found to protect cells from ischemia injury in the heart and brain via the δ receptors. On the other hand, κ antagonist prevents neurodegeneration.

The µ opioid receptors are localized predominately in the hypothalamus and thalamus, and the δ opioid receptors are localized predominately in the striatum, limbic system, and cerebral cortex (6, 7). The κ opioid receptors (κ_1_ and κ_2_ ) are the most abundant brain opioid receptors and are widely distributed in deeper layers of the neocortex (particularly temporal, parietal, and frontal cortices), striatum, amygdala, and thalamus, with lower levels in the hippocampus, occipital cortex, and cerebellum (8-10). The κ opioid receptors have been implicated in several clinical brain disorders, including drug abuse (11), epilepsy (12), Tourette’s syndrome (13), and Alzheimer’s disease (14).

Diprenorphine is a highly potent and nonselective opioid receptors antagonist with subnanomolar affinity (7). Diprenorphine has been labeled as [6-O-methyl-^11^C]diprenorphine ([^11^C]DPN) (15, 16). [^11^C]DPN is being developed as a PET agent for the non-invasive study of opioid receptors in the brain.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20diprenorphine%20and%20synthesis)]

Lever et al. (15) reported synthesis of [6-O-methyl-^11^C]diprenorphine by [^11^C]-O-methylation of 3-O-t-butyldimethylsilyl-(6-O-desmethyl)diprenorphine with [^11^C]methyl iodide , and final acidic deprotection of the product. An average radiochemical yield was 10% with a total synthesis time of 30 min. An average specific activity was 64 GBq/μmol (1.74 Ci/μmol at end of synthesis) with a radiochemical purity of >98%.

Luthra et al. (16) reported an automated radiosynthesis of [6-O-methyl-^11^C]diprenorphine by

O-methylation of (3-O-trityl,6-desmethyl)diprenorphine with [^11^C]iodomethane in the presence of NaH in DMF, following by de-protection acid hydrolysis. The two-step reaction provided [^11^C]DPN in a 13–19% radiochemical yield with a specific activity of 15.5–23.8 GBq/μmol (0.41-0.64 Ci/μmol) at end of synthesis. The preparation takes 45 min from end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20diprenorphine%20and%20in%20vitro)]

Chang et al. (6) reported that [^3^H]DPN had a K_d_ of 0.23 nM and a B_max_ of 530 fmol/mg protein in vitro binding assays using rat brain membranes. DPN had K_i_ values of 0.20, 0.18, and 0.47 nM for the µ, δ, and κ opioid receptors, respectively. Therefore, DPN binds to all three subtypes of opioid receptors equally with good affinity.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20diprenorphine%20and%20rodentia)]

Biodistribution studies in rats injected with 18.5 MBq (0.5 mCi) [^11^C]DPN were performed by Rajeswaran et al. (17) showing high accumulation of radioactivity in the thalamus and caudate putamen at 40 min post injection. Brain region to cerebellum ratios increased over time with ratios at 40 min of 8.6 and 7.2 for the thalamus and caudate putamen, respectively. Pretreatment with naloxone (an opioid receptor competitive antagonist) decreased both ratios to ~2. The cerebellum had low activity because of more rapid washout. Naloxone also blocked the cerebellum uptake from 0.26 to 0.14, indicating there are a few opioid receptors. The accumulation of radioactivity in the striatum and cerebellum and their blocking with DPN (200 ng/kg) and naloxone (1 mg/kg) pretreatment were confirmed by PET imaging in another experiment.

Shiue et al. (18) demonstrated a high accumulation of [^11^C]DPN in the mouse brain (1.2% injected dose) at 30 min after injection. The fraction of unchanged [^11^C]DPN in the brain determined by HPLC was 82-89% at 30 min after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20diprenorphine%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20diprenorphine%20and%20%28primate%20not%20human%29)]

Shiue et al. (18) studied two adult female baboons with [^11^C]DPN PET imaging under baseline conditions and after pretreatment with naloxone (1 mg/kg). Four parameter constants (k_1_-k_4_) were derived from PET scan data using Logan analysis with arterial input function. The three regions of interest were the striatum, thalamus, and cerebellum. High levels of [^11^C]DPN radioactivity were found in all three regions initially. However, the radioactivity in the cerebellum was washed out faster than the striatum and thalamus. The striatum/cerebellum ratio was 3.2 at 90 min. Pretreatment with naloxone blocked the accumulation of [^11^C]DPN radioactivity in the striatum and thalamus more significantly than in the cerebellum. The fraction of unchanged [^11^C]DPN in plasma samples determined by HPLC was 63% at 20 min and 28% at 60 min after injection.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20diprenorphine%20and%20human)]

Sadzot et al. (19) reported PET studies in human brain using high and low specific activity [^11^C]DPN. Non-steady-state three-compartment modeling and non-linear least-squares curve fitting were performed to obtain in vivo estimates of B_max_ and K_d_ in eight brain regions. The B_max_ values were from 2.3 ± 0.5, 6.8 ± 2.1, 12.0 ± 3.7, 13.1 ± 3.6, 13.4 ± 2.6, 18.6 ± 1.9, 19.9 ± 10.0, 20.5 ± 7.3 nM in the occipital cortex, cerebellum, parietal cortex, frontal cortex, temporal cortex, thalamus, caudate, and cingulated cortex, respectively. The averaged K_d_ from the eight brain regions was 0.85 ± 0.17 nM. Binding potentials and volumes of distribution can also be estimated using only high specific activity [^11^C]DPN and the occipital cortex as a reference region. Pretreatment with 1 mg/kg naloxone, the uptake of [^11^C]DPN was reduced to background levels throughout the brain.

Jones et al. (20, 21) performed [^11^C]DPN PET studies endogenous opiate response to pain (in and out of pain) in patients with rheumatoid arthritis (n = 4). There were significant increases in [^11^C]DPN binding in association with a reduction in pain in most of the areas of the brain that were sampled apart from the occipital cortex, such as in the frontal cortex, cingulate cortex, temporal cortex, and straight gyrus. Jones et al. (22) and Willoch et al. (23) also found there were decreases in [^11^C]DPN binding in various cerebral cortices and the thalamus in patients with poststroke pain. These findings suggest that there are substantial increases in opioid receptor occupancy by endogenous opioid peptides during pain.

Weeks et al. (24) compared regions of interest (ROIs) analytical approaches with statistical parametric mapping (SPM) of [^11^C]DPN PET findings in five patients with Huntington's disease (HD) and nine age-matched controls. The ROIs were placed on the caudate, putamen and occipital reference. Ratios of striatal-occipital uptake from averaged static images centered at 60 minutes showed an average of 20% reduction of [^11^C]DPN receptor binding in the caudate (P = 0.034) and 15% reduction in the putamen (P = 0.095) in the HD patients. Studies performed with SPM revealed symmetrical [^11^C]DPN binding decreases in the caudate (peak 40% decrease) and putamen (peak 24% decrease) with also decreases in the cingulated (peak 48% decrease), prefrontal (peak 13% decrease), and thalamic (peak 19% decrease) regions. Using these two approaches, Piccini et al. (25) found significantly reduction of [^11^C]DPN opioid binding in the striatum and thalamus in levodopa-induced dyskinetic, but not in nondyskinetic, Parkinson’s disease (PD) patients by using the ROI approach. The SPM approach confirmed reduced availability in these areas and, in addition, showed decreased cingulate and increased prefrontal opioid receptor binding in the dyskinetic PD patients. Burn et al. (26) has reported previously that there were no significant decreases in [^11^C]DPN binding in the caudate and putamen of eight PD patients compared with eight normal controls.

Mayberg et al. (27) reported that [^11^C]DPN binding was not significantly different among regions in the focus and nonfocus temporal lobes in eleven patients with epilepsy. However, Koepp et al. (28) reported that [^11^C]DPN binding to opioid receptors was significantly lower (P<0.05) in the left parieto-temporo-occipital cortex in five reading-epilepsy patients compared with six age-matched controls. Therefore, endogenous opioid peptides were released in localized areas of the brain during seizures induced by reading.

Internal dosimetry data for [^11^C]DPN in humans are not available in the literature.

## References

1 Minami M., Satoh M. (1995). Molecular biology of the opioid receptors: structures, functions and distributions. Neurosci Res.
2 Waldhoer M., Bartlett S.E., Whistler J.L. (2004). Opioid receptors. Annu Rev Biochem.
3 Satoh M., Minami M. (1995). Molecular pharmacology of the opioid receptors. Pharmacol Ther.
4 Molina P.E. (2006). Opioids and opiates: analgesia with cardiovascular, haemodynamic and immune implications in critical illness. J Intern Med.
5 Barry U., Zuo Z. (2005). Opioids: old drugs for potential new applications. Curr Pharm Des.
6 Chang K.J., Cooper B.R., Hazum E., Cuatrecasas P. (1979). Multiple opiate receptors: different regional distribution in the brain and differential binding of opiates and opioid peptides. Mol Pharmacol.
7 Pfeiffer A., Pasi A., Mehraein P., Herz A. (1982). Opiate receptor binding sites in human brain. Brain Res.
8 Peckys D., Landwehrmeyer G.B. (1999). Expression of mu, kappa, and delta opioid receptor messenger RNA in the human CNS: a 33P in situ hybridization study. Neuroscience.
9 Hiller J.M., Fan L.Q. (1996). Laminar distribution of the multiple opioid receptors in the human cerebral cortex. Neurochem Res.
10 Simonin F., Gaveriaux-Ruff C., Befort K., Matthes H., Lannes B., Micheletti G., Mattei M.G., Charron G., Bloch B., Kieffer B. (1995). kappa-Opioid receptor in humans: cDNA and genomic cloning, chromosomal assignment, functional expression, pharmacology, and expression pattern in the central nervous system. Proc Natl Acad Sci U S A.
11 Mello N.K., Negus S.S. (2000). Interactions between kappa opioid agonists and cocaine. Preclinical studies. Ann N Y Acad Sci.
12 de Lanerolle N.C., Williamson A., Meredith C., Kim J.H., Tabuteau H., Spencer D.D., Brines M.L. (1997). Dynorphin and the kappa 1 ligand [3H]U69,593 binding in the human epileptogenic hippocampus. Epilepsy Res.
13 Chappell P.B., Leckman J.F., Scahill L.D., Hardin M.T., Anderson G., Cohen D.J. (1993). Neuroendocrine and behavioral effects of the selective kappa agonist spiradoline in Tourette's syndrome: a pilot study. Psychiatry Res.
14 Mathieu-Kia A.M., Fan L.Q., Kreek M.J., Simon E.J., Hiller J.M. (2001). Mu-, delta- and kappa-opioid receptor populations are differentially altered in distinct areas of postmortem brains of Alzheimer's disease patients. Brain Res.
15 Lever J.R., Dannals R.F., Wilson A.A., Ravert H.T., Wagner H.N. (1987). Synthesis of carbon-11 labeled diprenorphine: a radioligand for positron emission tomographic studies of opiate receptors. Tetrahedron Letters.
16 Luthra S.K., Brady F., Turton D.R., Brown D.J., Dowsett K., Waters S.L., Jones A.K., Mathews R.W., Crowder J.C. (1994). Automated radiosyntheses of [6-O-methyl-11C]diprenorphine and [6-O-methyl-11C]buprenorphine from 3-O-trityl protected precursors. Appl Radiat Isot.
17 Rajeswaran S., Hume S.P., Cremer J.E., Young J., Bailey D.L., Ashburner J., Luthra S.K., Jones A.K., Jones T. (1991). Dynamic monitoring of [11C]diprenorphine in rat brain using a prototype positron imaging device. J Neurosci Methods.
18 Shiue C.Y., Bai L.Q., Teng R.R., Arnett C.D., Dewey S.L., Wolf A.P., McPherson D.W., Fowler J.S., Logan J., Holland M.J., et al. (1991). A comparison of the brain uptake of N-(cyclopropyl[11C]methyl)norbuprenorphine ([11C]buprenorphine) and N-(cyclopropyl[11C]methyl)nordiprenorphine ([11C]diprenorphine) in baboon using PET. Int J Rad Appl Instrum B.
19 Sadzot B., Franck G. (1990). Non-invasive methods to study drug disposition: positron emission tomography. Detection and quantification of brain receptors in man. Eur J Drug Metab Pharmacokinet.
20 Jones A.K., Cunningham V.J., Ha-Kawa S., Fujiwara T., Luthra S.K., Silva S., Derbyshire S., Jones T. (1994). Changes in central opioid receptor binding in relation to inflammation and pain in patients with rheumatoid arthritis. Br J Rheumatol.
21 Jones A.K., Liyi Q., Cunningham V.V., Brown D.W., Ha-Kawa S., Fujiwara T., Friston K.F., Silva S., Luthra S.K., Jones T. (1991). Endogenous opiate response to pain in rheumatoid arthritis and cortical and subcortical response to pain in normal volunteers using positron emission tomography. Int J Clin Pharmacol Res.
22 Jones A.K., Watabe H., Cunningham V.J., Jones T. (2004). Cerebral decreases in opioid receptor binding in patients with central neuropathic pain measured by [11C]diprenorphine binding and PET. Eur J Pain.
23 Willoch F., Schindler F., Wester H.J., Empl M., Straube A., Schwaiger M., Conrad B., Tolle T.R. (2004). Central poststroke pain and reduced opioid receptor binding within pain processing circuitries: a [11C]diprenorphine PET study. Pain.
24 Weeks R.A., Cunningham V.J., Piccini P., Waters S., Harding A.E., Brooks D.J. (1997). 11C-diprenorphine binding in Huntington's disease: a comparison of region of interest analysis with statistical parametric mapping. J Cereb Blood Flow Metab.
25 Piccini P., Weeks R.A., Brooks D.J. (1997). Alterations in opioid receptor binding in Parkinson's disease patients with levodopa-induced dyskinesias. Ann Neurol.
26 Burn D.J., Rinne J.O., Quinn N.P., Lees A.J., Marsden C.D., Brooks D.J. (1995). Striatal opioid receptor binding in Parkinson's disease, striatonigral degeneration and Steele-Richardson-Olszewski syndrome, A [11C]diprenorphine PET study. Brain.
27 Mayberg H.S., Sadzot B., Meltzer C.C., Fisher R.S., Lesser R.P., Dannals R.F., Lever J.R., Wilson A.A., Ravert H.T., Wagner H.N., et al. (1991). Quantification of mu and non-mu opiate receptors in temporal lobe epilepsy using positron emission tomography. Ann Neurol.
28 Koepp M.J., Richardson M.P., Brooks D.J., Duncan J.S. (1998). Focal cortical release of endogenous opioids during reading-induced seizures. Lancet.